# [^125^I]N-[2-[N-Ethyl-N-[2-(2-fluoropyridin-3-yloxy)ethyl]amino]ethyl]-6-iodoquinoxaline-2-carboxamide dihydrochloride salt

Chemical name: | [^125^I]N-[2-[N-Ethyl-N-[2-(2-fluoropyridin-3-yloxy)ethyl]amino]ethyl]-6-iodoquinoxaline-2-carboxamide dihydrochloride salt | [image]
Abbreviated name: | [^125^I]56 | [image]
Synonym: | [^131^I]56 | [image]
Agent Category: | Compounds | [image]
Target: | Melanin | [image]
Target Category: | Others | [image]
Method of detection: | Single-photon emission computed tomography (SPECT), planar imaging | [image]
Source of signal / contrast: | ^125^I | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Chemical structure of [^125^I]56 (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=benzamide+and+imaging+and+therapy)]

Radioiodinated N-[2-[N-ethyl-N-[2-(2-fluoropyridin-3-yloxy)ethyl]amino]ethyl]-6-iodoquinoxaline-2-carboxamide dihydrochloride salt, abbreviated as [^125^I]56, is a quinoxaline benzamide (BZA) derivative that was synthesized for melanin-targeted radionuclide imaging and therapy of melanoma (1).

BZA derivatives represent a versatile class of aromatic compounds that possess a common structure element of Ph-CONH(CH_2_)_m_NR_2_ (m = 1, 2) and exhibit comparable properties, including high and specific binding with melanin in melanoma cells and melanocytes (2-4). Some of these compounds, such as N-(2-diethylaminoethyl)-4-[^123^I]iodobenzamide ([^123^I]BZA) and [^123^I]-N-(2-diethylaminoethyl)-2-iodobenzamide ([^123^I]BZA2), have been successfully evaluated in melanoma patients, showing high sensitivity and selectivity in the detection of melanoma and its metastases (5-8).

The promising results with [^123^I]BZA have prompted great efforts from several groups in screening BZA analogs (2, 9, 10). Among them is a group of investigators in France who synthesized a series of BZA derivatives via structure-activity studies (11, 12). On the basis of the structure of the lead agent [^123^I]BZA, they synthesized a group of spermidine BZA derivatives by replacing the diethylaminoethyl moiety in the BZA structure with a triamine (spermidine). Spermidine BZA derivatives exhibit high affinity for melanin comparable to that of [^123^I]BZA; however, these compounds exhibit less accumulation in tumors than [^123^I]BZA in animal models of melanoma (13). More recently, the investigators generated a class of heteroaromatic BZA analogs by incorporating the heteroaromatic structure in place of the benzene moiety to take advantage of the polycyclic aromatic compounds that display a strong affinity for melanin while keeping the lipophilic side chain (14). The heteroaromatic analogs, [^125^I]5a through [^125^I]5I, showed high specific and long-lasting uptake in the melanoma, which is favorable for combined imaging and therapy. At the same time, the investigators also identified a group of quinoxaline analogs; radioiodinated derivative 3 (ICF01012) is one of these compounds, which show the most favorable pharmacokinetic properties for radionuclide therapy (15, 16). The rapid and specific tumor uptake of quinoxaline compounds also suggests that they are potentially valuable for radionuclide imaging. For radiofluorination, ICF01012 was modified by incorporating 2- or 6-fluoropyridine in the N,N-diethylethylenediamine framework of ICF01012. This strategy allows nucleophilic heteroaromatic radiofluorination of corresponding halogeno- or nitro-precursors without the need for an additional electron-withdrawing substituent in the aromatic ring. Fluoropyridine was introduced on the tertiary amine either directly or in combination with various linkers, which resulted in a group of amide tracers, such as the agents [^125^I]56 and [^18^F]44 (compound 56 is the dihydrochloride salt of 44) (1). These derivatives showed favorable properties for combined radionuclide imaging (^18^F, ^125^I) and therapy (^131^I) of melanoma using a single chemical structure. The following is a list of some representative agents that were synthesized and tested by the investigators from the group in France.

BZA derivatives: [^125/123^I]BZA, [^125^I]BZA2, [^125^I]BZ18, and [^125^I]5a through [^125^I]5I; and quinoxaline derivatives: [^125/131^I]ICF01012 (or [^125/131^I]3), [^125^I]56, and [^18^F]44.

This chapter summarizes the data of imaging studies obtained with [^125^I]56 (1).

### Related Resource Links:

Melanin-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=melanin+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Benzamide derivatives in PubChem (http://www.ncbi.nlm.nih.gov/sites/entrez?db=pcsubstance&term=benzamide) Benzamide derivatives in clinical trials in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=benzamide)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21417462)]

Maisonial et al. described the chemical synthesis and characterization of compound 56 in detail (1). Compound 56 was synthesized starting from the corresponding stannane precursor 76 (N-[2-[N-ethyl-N-[2-(2-fluoropyridin-3-yloxy)ethyl]amino]ethyl]-6-tributylstannylquinoxaline-2-carboxamide). The formula of compound 56 was C_20_H_21_FIN_5_O_2_,2HCl,H_2_O. The chemical yield was 91%. Radiolabeled versions of compound 56, [^125^I]56 and [^131^I]56, were synthesized with a classic electrophilic radioiodo-demetalation reaction, using no-carrier-added [^125^I]NaI and [^131^I]NaI, respectively, in acidic medium (citrate buffer) in the presence of chloramine-T monohydrate. The radiochemical yield and purity of [^125^I]56 were 53% and 99.7%, respectively, and the specific activity was 31.9 GBq/μmol (0.86 Ci/µmol). [^131^I]56 was obtained with a specific activity of 106.9 GBq/μmol (2.89 Ci/µmol) and a radiochemical purity of 98.5%; the radiochemical yield of [^131^I]56 was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21417462)]

The in vitro data of the lead compound 3 were summarized in the literature regarding [^125^I]ICF01012 (or [^125^I]3) (15, 16). In vitro studies with cells were not performed for the compound 56.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21417462)]

Maisonial et al. performed a biodistribution study in C57B16 mice (n = 3) bearing melanoma B16F0 tumors after injection of 2.7 MBq (0.073 mCi) [^125^I]56, with [^125^I]3 as the reference (1). High tumor accumulation was observed at 1 h, and it increased gradually to a maximum at 3–6 h. The radioactivity continued to be measurable for at least 5 days. The tumor uptake levels were12.7 ± 2.3, 20.2 ± 4.2, 18.8 ± 1.6, 18.2 ± 0.6, 10.3 ± 1.7, 5.2 ± 1.2, 3.2 ± 0.4, 1.7 ± 0.4, 0.6 ± 0.3% injected dose per gram tissue (ID/g) at 1, 3, and 6 h and 1, 3, 5, 7, 10, and 14 days after injection, respectively. In comparison, the tumor uptake levels of [^125^I]3 were 21.8 ± 6.6, 26.3 ± 6.6, 29.6 ± 8.4, 28.0 ± 8.2, 12.3 ± 3.7, 7.3 ± 3.6, 3.4 ± 0.3, and 1.9 ± 0.4% ID/g 1, 3, and 6 h and 1, 3, 5, 7, and 10 days after injection. [^125^I]56 showed a rapid excretion (20% remaining after 24 h), similar to that observed with [^125^I]3. These results suggest that [^125^I]56 maintains the high tumor affinity, giving rapid and long-lasting tumor radioactivity uptake. The long-lasting tumor radioactivity uptake led to a calculated biological half-life of 38 h for [^131^I]56 and a tumor-absorbed dose of 1.12 Gy/MBq of injected [^131^I]56. Although these values were lower than those obtained with [^131^I]3 (49.3 h and 1.71 Gy/MBq injected), they were in a range compatible with radionuclide therapy for melanoma No blocking studies were performed.

Serial scintigraphic images also illustrated rapid clearance from nontarget organs, allowing well-defined images of the tumor. In nontarget organs of liver, lung, or kidney (n = 2 mice), radioactive uptake decreased to a very low level after 3 h and was undetectable after 24 h. The tumor/muscle ratios were 23 and 37 at 1 h and 3 h after injection, respectively. The pigmented structures of the eyes exhibited a radioactivity uptake profile similar to that of the tumor. High radioactive uptake was also visualized in the throat area, mainly in the salivary glands and thyroid, likely due to a nonspecific concentration. Analyses on collected urine and feces showed an imbalance between urinary and fecal elimination routes, at 38.1% and 36.1%, respectively, for the 0−24 h period and 45.1% and 38.7%, respectively, for the 0−72 h period.

The therapeutic efficacy of [^131^I]56 was assessed in C57B16 mice bearing subcutaneous B16F0 melanoma (n = 10 mice). Two doses of [^131^I]56 (2 × 18.5 MBq) were administered at day 6 and day 10, respectively. B16F0 tumors in the untreated group (n = 10 mice) showed exponential growth, with a tumor-doubling time of 2.8 ± 0.3 days, whereas [^131^I]56 inhibited the in vivo growth of B16F0 tumors (doubling time, 3.8 ± 0.3 days) (P < 0.001). The concentration of [^131^I]56 used here was much lower than its 50% lethal dose (data not shown).

In summary, Maisonial et al. synthesized 14 new iodinated and fluorinated analogs of the lead compound 3 ([^131^I]3) (1). All of these tracers contain a 2- or 6-fluoropyridine moiety incorporated in the N,N-diethylethylenediamine scaffold. Most of these novel radioiodinated compounds showed significant tumor retention, especially the derivative [^125/131^I]56, which presented high and long-lasting tumor uptake combined with a rapid clearance from nontarget organs, offering both diagnostic (^125^I and ^18^F) and therapeutic (^131^I) potentialities (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Maisonial A., Kuhnast B., Papon J., Boisgard R., Bayle M., Vidal A., Auzeloux P., Rbah L., Bonnet-Duquennoy M., Miot-Noirault E., Galmier M.J., Borel M., Askienazy S., Dolle F., Tavitian B., Madelmont J.C., Moins N., Chezal J.M. (2011). Single photon emission computed tomography/positron emission tomography imaging and targeted radionuclide therapy of melanoma: new multimodal fluorinated and iodinated radiotracers. J Med Chem.
2 Oltmanns D., Eisenhut M., Mier W., Haberkorn U. (2009). Benzamides as melanotropic carriers for radioisotopes, metals, cytotoxic agents and as enzyme inhibitors. Curr Med Chem.
3 Chehade F., De Labriolle-Vaylet C., Michelot J., Moins N., Moreau M.F., Hindie E., Papon J., Escaig F., Galle P., Veyre A. (2001). Distribution of I-BZA (N-2-diethylaminoethyl-4-iodobenzamide) in grafted melanoma and normal skin: a study by secondary ion mass spectroscopy. Cell Mol Biol (Noisy-le-grand).
4 Greguric I., Taylor S.R., Denoyer D., Ballantyne P., Berghofer P., Roselt P., Pham T.Q., Mattner F., Bourdier T., Neels O.C., Dorow D.S., Loc'h C., Hicks R.J., Katsifis A. (2009). Discovery of [18F]N-(2-(diethylamino)ethyl)-6-fluoronicotinamide: a melanoma positron emission tomography imaging radiotracer with high tumor to body contrast ratio and rapid renal clearance. J Med Chem.
5 Bacin F., Michelot J., Bonafous J., Veyre A., Moreau M.F., Kemeny J.L., Chossat F., Bekhechi D. (1998). Clinical study of [123I] N-(2-diethylaminoethyl)-4-iodobenzamide in the diagnosis of primary and metastatic ocular melanoma. Acta Ophthalmol Scand.
6 Michelot J.M., Moreau M.F., Veyre A.J., Bonafous J.F., Bacin F.J., Madelmont J.C., Bussiere F., Souteyrand P.A., Mauclaire L.P., Chossat F.M., et al. (1993). Phase II scintigraphic clinical trial of malignant melanoma and metastases with iodine-123-N-(2-diethylaminoethyl 4-iodobenzamide). J Nucl Med.
7 Mansard S., Papon J., Moreau M.F., Miot-Noirault E., Labarre P., Bayle M., Veyre A., Madelmont J.C., Moins N. (2005). Uptake in melanoma cells of N-(2-diethylaminoethyl)-2-iodobenzamide (BZA2), an imaging agent for melanoma staging: relation to pigmentation. Nucl Med Biol.
8 Moins N., D'Incan M., Bonafous J., Bacin F., Labarre P., Moreau M.F., Mestas D., Noirault E., Chossat F., Berthommier E., Papon J., Bayle M., Souteyrand P., Madelmont J.C., Veyre A. (2002). 123I-N-(2-diethylaminoethyl)-2-iodobenzamide: a potential imaging agent for cutaneous melanoma staging. Eur J Nucl Med Mol Imaging.
9 Labarre P., Papon J., Moreau M.F., Moins N., Bayle M., Veyre A., Madelmont J.C. (2002). Melanin affinity of N-(2-diethylaminoethyl)-4-iodobenzamide, an effective melanoma imaging agent. Melanoma Res.
10 Moins N., Papon J., Seguin H., Gardette D., Moreau M.F., Labarre P., Bayle M., Michelot J., Gramain J.C., Madelmont J.C., Veyre A. (2001). Synthesis, characterization and comparative biodistribution study of a new series of p-iodine-125 benzamides as potential melanoma imaging agents. Nucl Med Biol.
11 Desbois N., Gardette M., Papon J., Labarre P., Maisonial A., Auzeloux P., Lartigue C., Bouchon B., Debiton E., Blache Y., Chavignon O., Teulade J.C., Maublant J., Madelmont J.C., Moins N., Chezal J.M. (2008). Design, synthesis and preliminary biological evaluation of acridine compounds as potential agents for a combined targeted chemo-radionuclide therapy approach to melanoma. Bioorg Med Chem.
12 Labarre P., Papon J., Rose A.H., Guerquin-Kern J.L., Morandeau L., Wu T.D., Moreau M.F., Bayle M., Chezal J.M., Croisy A., Madelmont J.C., Turner H., Moins N. (2008). Melanoma affinity in mice and immunosuppressed sheep of [(125)I]N-(4-dipropylaminobutyl)-4-iodobenzamide, a new targeting agent. Nucl Med Biol.
13 Moreau M.F., Papon J., Labarre P., Moins N., Borel M., Bayle M., Bouchon B., Madelmont J.C. (2005). Synthesis, in vitro binding and biodistribution in B16 melanoma-bearing mice of new iodine-125 spermidine benzamide derivatives. Nucl Med Biol.
14 Chezal J.M., Papon J., Labarre P., Lartigue C., Galmier M.J., Decombat C., Chavignon O., Maublant J., Teulade J.C., Madelmont J.C., Moins N. (2008). Evaluation of radiolabeled (hetero)aromatic analogues of N-(2-diethylaminoethyl)-4-iodobenzamide for imaging and targeted radionuclide therapy of melanoma. J Med Chem.
15 Bonnet M., Mishellany F., Papon J., Cayre A., Penault-Llorca F., Madelmont J.C., Miot-Noirault E., Chezal J.M., Moins N. (2010). Anti-melanoma efficacy of internal radionuclide therapy in relation to melanin target distribution. Pigment Cell Melanoma Res.
16 Bonnet-Duquennoy M., Papon J., Mishellany F., Labarre P., Guerquin-Kern J.L., Wu T.D., Gardette M., Maublant J., Penault-Llorca F., Miot-Noirault E., Cayre A., Madelmont J.C., Chezal J.M., Moins N. (2009). Targeted radionuclide therapy of melanoma: anti-tumoural efficacy studies of a new 131I labelled potential agent. Int J Cancer.